# Cross-linked iron oxide-Cy5.5

Chemical name: | Cross-linked iron oxide-Cy5.5
Abbreviated name: | CLIO-Cy5.5
Synonym:
Agent Category: | Iron oxide
Target: | Phagocyte and tumor cell
Target Category: | Endocytosis
Method of detection: | Magnetic resonance (MRI), Optical (NIRF)
Source of signal: | Iron oxide, Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO%20Cy5.5)]

Complete resection is critical in terms of survival of brain tumor populations (1). Consequently, accurate delineation of tumor margins is critical to the successful surgical resection of brain tumors. It is important to relate the preoperative radiological images to the visual presentation of pathology during surgery. There are several such visible wavelength-emitting optical agents as fluorecein (2), indocyanine green (3), and porphyrin (4, 5) have been used to provide intraoperative fluorescence images in the tumor region. However, they have not been widely accepted as providing accurate tumor boundary because of the limited circulation time, mediocre signal-to-noise ratio, and readily diffuse into and out of the interstitial space. Other low molecular weight agents such as gadolinium chelates have been applied to obtain the contrast-enhanced magnetic resonance (MR) image, but they were not very useful intraoperatively because the distribution was not constant over the hours required by tumor resection. Hence it is of interest to develop a reagent that provides preoperative MR image which can be visualized intraoperatively.

A multimodal nanoparticle probe that consists of a contrasting agent (for preoperative MR image) and a near infrared (NIR) fluorochrome (for intraoperative visualization) may provide consistent information both preoperatively and intraoperatively. Superparamagnetic iron oxide nanoparticles such as MION and CLIO can be internalized by cells of reticuloendothelial system and have long circulating time within animal body. Therefore, it can accumulate in the brain tumors (6). The blood half-life of MION in human is about 24 hours (7) and the blood half-lives of both CLIO-NH_2_ and MION are about 10 hours in mice (8). The accumulation of nanoparticles in cells cause reduction in signal intensity with T2-weighted spin echo pulse sequences. These nanoparticles thus become a good choice to be administered before the surgery for MR images. Compare to visible wavelength-emitting fluorochromes, NIR fluorochrome (e.g. Cy5.5) provides improved light transmission through tissue and decreases the effect, hence the background, of autofluorescence from brain tissue (9). Near Infrared fluorescence (NIRF) also provides simultaneous full-color spectrum white light imaging while acquiring and displaying fluorescence separately (10).

CLIO-Cy5.5 (1, 9) is a multimodal agent that consists of a superparamagnetic iron oxide nanoparticle (CLIO) and a NIR fluorochrome (Cy5.5). It serves as a contrast agent for preoperative MRI to visualize the brain tumor and, in the meantime, provides an intraoperative NIR fluorescence image that discriminate tumor from normal brain tissue because of the phagocytic function of tumor cells. This nanoparticle is internalized by cells before surgery begins and does not diffuse out of the cells or through the interstitial space during the surgery, consequently, it could be a useful agent which provides consistent information before and during the brain tumor resection.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO%20MRI%20Cy5.5)]

The synthesis of CLIO-Cy5.5 was described by Kircher et al. (9). In brief, 0.2 mL of CLIO-NH_2_ nanoparticle (produced by mixing CLIO nanoparticles with dextran, followed by activation with epichlorohydrin and ammonia (11, 12), at a concentration of 10 mg Fe/mL in a citrate buffer (20 mM, pH 8) was mixed with Cy5.5 solution at room temperature for 2 h, followed by incubation at 4°C overnight. Excess Cy5.5 was removed by gel filtration using a Sephadex G-25 column in a citrate buffer (20 mM, 150mM NaCl, pH 8). The size of the nanoparticle was determined to be 32 nm using laser light scattering method and had an average of 1 Cy5.5 dye per iron oxide crystal.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO%20Cy5.5%20in%20vitro)]

No relevant publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO%20Cy5.5%20rodentia)]

The study of brain tumor delineation by CLIO-Cy5.5 was performed by injecting the 9L rat gliosarcoma cell line transfected to express GFP (9L-GFP-cell) into Fischer 344 rats (9). MRI of rat was performed 10-14 days after tumor inoculation. Cy5.5-CLIO (15 mg/kg) was introduced into animals through tail vein injection and MRI was performed 24 h after the injection. The distribution of tumor in the brain was determined by fluorescence of GFP and Cy5.5 on the cryosectioned tumors. High congruency of tumor extent was observed between the MR image and the H&E staining. The accumulation of iron was demonstrated by DAB-amplified Prussian blue stain. Twenty-five slices of five brain tumors were analyzed by comparing both Cy5.5 and GFP positive area. The data was fitted with linear regression. It showed a slope of 1.013, and intercept of 0.820 mm^2^, and a R^2^ of 0.996. The over estimation by Cy5.5 compared to the tumor delineation by GFP fluorescence was caused by the uptake of CLIO-Cy5.5 by microglia.

Hosts with different immune responses to the tumor were used to further asses the accuracy of brain tumor delineation by CLIO-Cy5.5. GFP expressing tumor cells were implanted in Wistar male rate and female nude mice (1). Images were taken after 7-10 days of inoculation. CLIO-Cy5.5 (15 mg/kg) was administered through tail vein injection and MR images were taken 24 h after the introduction of CLIO-Cy5.5. A threshold method was applied to determine the boundary of tumors. The average overestimation of CLIO-Cy5.5 border was 0.02 mm in the rat and 0.002 mm in nude mouse compared to the GFP border (which indicated the tumor extent). The maximum overestimation was 65 and 151 μm, respectively, and the maximum underestimation was 64 and 57 μm, respectively, for mice and rat. These were within a few cell diameters of the true tumor boundary. CLIO-Cy5.5 nanoparticles were internalized by microglia/macrophages at the periphery of the tumor and the tumor cells. There was no uptake of the nanoparticle by astrocytes.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO%20Cy5.5%20%28dog%20or%20sheep%20or%20pig%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO%20AND%20Cy5.5%20AND%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO%20AND%20Cy5.5%20AND%20human)]

No relevant publication is currently available.

## References

1 Trehin R, Figueiredo JL, Pittet MJ, Weissleder R, Josephson L, Mahmood U. (2006). Fluorescent nanoparticle uptake for brain tumor visualization. Neoplasia.
2 Kabuto M, Kubota T, Kobayashi H, Nakagawa T, Ishii H, Takeuchi H, Kitai R, Kodera T. (1997). Experimental and clinical study of detection of glioma at surgery using fluorescent imaging by a surgical microscope after fluorescein administration. Neurol Res.
3 Haglund MM, Berger MS, Hochman DW. (1996). Enhanced optical imaging of human gliomas and tumor margins. Neurosurgery.
4 Stummer W, Reulen HJ, Novotny A, Stepp H, Tonn JC. (2003). Fluorescence-guided resections of malignant gliomas--an overview. Acta Neurochir Suppl (Wien).
5 Stummer W, Stocker S, Wagner S, Stepp H, Fritsch C, Goetz C, Goetz AE, Kiefmann R, Reulen HJ. (1998). Intraoperative detection of malignant gliomas by 5-aminolevulinic acid-induced porphyrin fluorescence. Neurosurgery.
6 Varallyay P, Nesbit G, Muldoon LL, Nixon RR, Delashaw J, Cohen JI, Petrillo A, Rink D, Neuwelt EA. (2002). Comparison of two superparamagnetic viral-sized iron oxide particles ferumoxides and ferumoxtran-10 with a gadolinium chelate in imaging intracranial tumors. AJNR Am J Neuroradiol.
7 McLachlan SJ, Morris MR, Lucas MA, Fisco RA, Eakins MN, Fowler DR, Scheetz RB, Olukotun AY. (1994). Phase I clinical evaluation of a new iron oxide MR contrast agent. J Magn Reson Imaging.
8 Wunderbaldinger P, Josephson L, Bremer C, Moore A, Weissleder R. (2002). Detection of lymph node metastases by contrast-enhanced MRI in an experimental model. Magn Reson Med.
9 Kircher MF, Mahmood U, King RS, Weissleder R, Josephson L. (2003). A multimodal nanoparticle for preoperative magnetic resonance imaging and intraoperative optical brain tumor delineation. Cancer Res.
10 Funovics MA, Weissleder R, Mahmood U. (2004). Catheter-based in vivo imaging of enzyme activity and gene expression: feasibility study in mice. Radiology.
11 Josephson L, Perez JM, Weissleder R. (2001). Magnetic Nanosensors for the Detection of Oligonucleotide Sequences. Angew Chem Int Ed.
12 Josephson L, Tung CH, Moore A, Weissleder R. (1999). High-efficiency intracellular magnetic labeling with novel superparamagnetic-Tat peptide conjugates. Bioconjug Chem.